# ^99m^Tc-Labeled 1-hydroxy-2-(2-ethyl-4-methyl-1H-imidazol-1-yl)ethane-1,1-diyldiphosphonic acid

Chemical name: | ^99m^Tc-Labeled 1-hydroxy-2-(2-ethyl-4-methyl-1H-imidazol-1-yl)ethane-1,1-diyldiphosphonic acid
Abbreviated name: | [^99m^Tc]-EMIDP
Synonym:
Agent Category: | Compound
Target: | Bone (hydroxyapatite); farnesyl disphosphate (pyrophosphate) synthase (molecular target)
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals | Click on the above proposed structure of [^99m^Tc]-EMIDP (1) for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs) labeled with technetium ([^99m^Tc]-BP) are often used for bone scintigraphy to detect osteoporosis and other skeletal-related events (SREs), including bone metastases (1). These chemicals are known to promote osteoclast apoptosis and have a strong affinity for hydroxyapatite, a component of the bone matrix. The mechanism of action of these bone-seeking compounds is described in detail elsewhere (2, 3). Bone scintigraphy is usually performed 2–6 h after intravenous injection of a [^99m^Tc]-BP, resulting in exposure of the patient to radiation for an extended time. To develop BPs that are more efficient and require only a short waiting time before bone scintigraphy, investigators generated various BPs, including zoledronic acid (http://www.pharma.us.novartis.com/product/pi/pdf/Zometa.pdf) (ZL), which contains an imidazole group in its structure, and evaluated their efficacy for the treatment of various bone-related diseases (4, 5). ZL was determined to be the most potent BP available for treating bone resorption and is approved by the United States Food and Drug Administration (FDA) for the treatment of various tumor-induced SREs (6).

In an effort to further improve the potency of ZL, the imidazole group of the compound was modified to obtain 1-hydroxy-2-(2-ethyl-4-methyl-1H-imidazol-1-yl)ethane-1,1-diyldiphosphonic acid (EMIDP), and the chemical was labeled with ^99m^Tc to produce [^99m^Tc]-EMIDP (1). Subsequently, the biodistribution of [^99m^Tc]-EMIDP was studied in normal mice, and the radiochemical was evaluated as a bone-imaging agent in rabbits.

### Other sources of information:

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Farnesyl+diphosphate+synthase++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=diphosphonates) with bisphosphonates (or diphosphonates)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=emidp%5BAll%20Fields%5D&cmd=DetailsSearch)]

The synthesis and optimization of reaction conditions for labeling EMIDP with ^99m^Tc have been described by Lin et al. (1). The radiochemical purity of the tracer was reported to be >95% as determined with paper chromatography, and it had an Rf value between 0.9 and 1.0. The radiochemical yield of the reaction, specific activity, and final formulation of the labeled compound were not reported.

In another study, ^99m^Tc-labeled methylene diphosphonate ([^99m^Tc]-MDP) was compared with [^99m^Tc]-EMIDP as an imaging agent (1). However, the source, synthesis, radiochemical yield and purity, and specific activity of [^99m^Tc]-MDP were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=emidp&cmd=DetailsSearch)]

^99m^Tc-EMIDP was reported to maintain a radiochemical purity of >95% for at least 6 h at room temperature under in vitro conditions (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=emidp&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-EMIDP was studied in normal mice after intravenous injection of the labeled compound through the tail vein (1). The animals (n = 5 mice/time point) were euthanized at various time points ranging from 5 min to 240 min post-injection (p.i.) to harvest the major organs, including bone, and to determine the amount of accumulated radioactivity in the various tissues. The level of radioactivity in the bone was 3.29 ± 0.53% injected dose per gram tissue (% ID/g) at 5 min, increased to 7.07 ± 0.59% ID/g at 60 min, and decreased to 3.76 ± 0.20% ID/g by 240 min p.i. During the same period, radioactivity in the blood decreased from 10.00 ± 0.68% ID/g at 5 min to 0.17 ± 0.08% ID/g at 240 min p.i., and a similar trend was noted with the kidneys (10.58 ± 0.52% ID/g and 1.03 ± 0.07% ID/g at 5 min and 240 min p.i., respectively). All other organs showed an accumulation of the tracer between 0.36 ± 0.04% ID/g (brain) and 4.51 ± 0.12% ID/g (lungs) at 5 min p.i., which decreased to between 0.01 ± 0.00% ID/g (brain) and 0.22 ± 0.02% ID/g (lungs) at 240 min p.i. From this study it was clear that the radioactivity from [^99m^Tc]-EMIDP accumulated primarily in the bone and was cleared rapidly from all other soft tissues. No blocking studies were performed and no data was presented to show that the binding of [^99m^Tc]-EMIDP was saturable.

Pharmacokinetic parameters were derived from the amount of radioactivity cleared from blood of the mice over time (1). The distribution (t_1/2α_) and elimination (t_1/2β_) half-lives of [^99m^Tc]-EMIDP were estimated to be 5.28 min and 59.07 min, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=emidp&cmd=DetailsSearch)]

Dynamic and static single-photon emission computed tomography (SPECT) was performed on New Zealand rabbits (anesthetized with ketamine and diazepam) injected with [^99m^Tc]-EMIDP through the marginal ear vein (1). Dynamic SPECT images of the bones and the soft tissue were obtained every 5 min p.i., and a series of static scans were collected from the animals starting at 90 min p.i. for up to 360 min p.i. Regions of interest were drawn directly on the composite scanning images to calculate the ratios of bone uptake to soft tissue uptake. For comparison, a similar procedure was performed with animals injected with [^99m^Tc]-MDP (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=MDP99mTc), an FDA approved bone-scanning radiochemical. Both tracers were reported to have a similar imaging profile in the rabbits and accumulated mainly in the skeletal tissue, kidneys, and urinary bladder. However, at 1 h p.i., compared to [^99m^Tc]-MDP the accumulation of [^99m^Tc]-EMIDP was higher in the bone than in the soft tissues. This indicated that [^99m^Tc]-EMIDP had a higher selectivity for the bone than [^99m^Tc]-MDP. In addition, the [^99m^Tc]-EMIDP uptake ratios of bone to heart, liver, kidney, muscle, and stomach at 10 min p.i. were shown to increase from 1.17, 0.60, 0.53, 3.44, and 2.93, respectively, to 1.76, 1.06, 1.23, 6.70, and 5.93, respectively, at 50 min, suggesting that [^99m^Tc]-EMIDP was rapidly cleared from the soft tissue but was stable in the bone.

From these studies, the investigators concluded that [^99m^Tc]-EMIDP had a selectivity for the skeletal tissue in rabbits superior to that of [^99m^Tc]-MDP. The investigators suggested that more studies with this radiochemical were necessary before it could be used for bone scintigraphy in humans (1).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mtc%20emidp%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mtc%20emidp%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lin J., Luo S., Chen C., Qiu L., Wang Y., Cheng W., Ye W., Xia Y. (2010). Preparation and preclinical pharmacological study on a novel bone imaging agent (99m)Tc-EMIDP. Appl Radiat Isot.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Zhang Y., Cao R., Yin F., Hudock M.P., Guo R.T., Krysiak K., Mukherjee S., Gao Y.G., Robinson H., Song Y., No J.H., Bergan K., Leon A., Cass L., Goddard A., Chang T.K., Lin F.Y., Van Beek E., Papapoulos S., Wang A.H., Kubo T., Ochi M., Mukkamala D., Oldfield E. (2009). Lipophilic bisphosphonates as dual farnesyl/geranylgeranyl diphosphate synthase inhibitors: an X-ray and NMR investigation. J Am Chem Soc.
4 Widler L., Jaeggi K.A., Glatt M., Muller K., Bachmann R., Bisping M., Born A.R., Cortesi R., Guiglia G., Jeker H., Klein R., Ramseier U., Schmid J., Schreiber G., Seltenmeyer Y., Green J.R. (2002). Highly potent geminal bisphosphonates. From pamidronate disodium (Aredia) to zoledronic acid (Zometa). J Med Chem.
5 Asikoglu M., Durak F.G. (2009). The rabbit biodistribution of a therapeutic dose of zoledronic acid labeled with Tc-99m. Appl Radiat Isot.
6 Smith M.R. (2008). Osteoclast targeted therapy for prostate cancer: bisphosphonates and beyond. Urol Oncol.